# 4-[^18^F]Fluorobenzoyl-C2A domain of synaptotagmin I-glutathione-S-transferase

Chemical name: | 4-[^18^F]Fluorobenzoyl-C2A domain of synaptotagmin I-glutathione-S-transferase
Abbreviated name: | 4-[^18^F]FB-C2A-GST
Synonym:
Agent category: | Protein
Target: | Anionic phospholipids
Target category: | Phospholipid
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=468888), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about annexin V.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C2A-GST)]

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, atherosclerosis, and chronic hepatitis, as well as in the biology of normal cells, such as epithelial cells and immune cells (1). During apoptosis, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. PS is also accessible for annexin V (or annexin A5) binding in necrosis because of disruption of the plasma membrane. Annexin V, a 36-kDa protein, binds to PS with high affinity (K_d_ = 7 nM). Annexin V has been radiolabeled with ^123^I and ^99m^Tc for single-photon emission computed tomography imaging and with ^124^I for positron emission tomography (PET) (2-4). Annexin V has been successfully labeled with ^18^F (^18^F-labeled annexin V (4-[^18^F]FBA (http://www.ncbi.nlm.nih.gov/books/NBK23247/))) and is currently being developed as a PET agent for imaging apoptosis as well as necrosis (5, 6). Cy5.5-Annexin V (http://www.ncbi.nlm.nih.gov/books/NBK23603/) has been evaluated as an optical probe in small animals. Annexin V-CLIO-Cy5.5 (AnxCLIO-Cy5.5 (http://www.ncbi.nlm.nih.gov/books/NBK23475/)) is a multimodal agent that consists of CLIO nanoparticles labeled with annexin V and Cy5.5 (7).

Synaptotagmins are integral membrane proteins of synaptic vesicles with calcium ion (Ca^2+^) binding domains (8). The C2A domain of synaptotagmin I (Syt1) binds two to three Ca^2+^ ions and also binds anionic phospholipids including PS. Calcium binding to Syt1 participates in triggering neurotransmitter release at the synapse. Davletov et al. (9) showed that C2A-glutathione-S-transferase (C2A-GST) fusion protein binds specifically Ca^2+^ and anionic phospholipids. ^99m^Tc-Labeled C2A-GST (^99m^Tc-C2A-GST) has been shown to target apoptotic cells in acute myocardial infarction and tumor models in vivo in animal studies (10-14). Wang et al. (15) prepared 4-[^18^F]fluorobenzoyl-C2A-GST (4-[^18^F]FB-C2A-GST) as a PET agent for imaging of apoptotic cells.

### Related Resource Links:

- Chapters in MICAD (Annexin V (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Annexin%20V+AND+micad%5Bbook%5D), phospholipids (http://www.ncbi.nlm.nih.gov/books?term=phospholipid%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Annexin V (http://www.ncbi.nlm.nih.gov/gene/308), synaptotagmin I (http://www.ncbi.nlm.nih.gov/gene/6857))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Annexin V (http://www.ncbi.nlm.nih.gov/omim/131230), synaptotagmin I (http://www.ncbi.nlm.nih.gov/omim/185605))
- Clinical trials (Annexin V (http://www.clinicaltrials.gov/ct2/results?term=Annexin+V+))
- Drug information in FDA (Annexin V (http://google2.fda.gov/search?q=annexin+V&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C2A-GST%20and%20synthesis)]

Wang et al. (15) prepared 4-[^18^F]FB-C2A-GST with a two-step synthesis. N-Succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB) was synthesized by coupling [^18^F]SFB to O-(N-succinimidyl)-tetramethyluronium tetrafluoroborate. [^18^F]SFB and C2A-GST (0.2 mg) in borate buffer (pH 8.4) were incubated for 20 min at room temperature. 4-[^18^F]FB-C2A-GST was purified with column chromatography with a radiochemical purity of >98%. At the end of synthesis, 30–160 MBq (0.8–4.3 mCi) 4-[^18^F]FB-C2A-GST (n = 6) was obtained for intravenous injection. The decay-corrected yield was 35%–40% based on [^18^F]SFB. The total synthesis time was ~120 min from the end of bombardment. The specific activity of 4-[^18^F]FB-C2A-GST was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C2A-GST%20and%20in%20vitro)]

Wang et al. (15) performed cell-binding assays with 4-[^18^F]FB-C2A-GST in apoptotic human Jurkat T cells treated with camptothecin. The apoptotic cells showed a 4.6 ± 0.6-fold higher radioactivity uptake than that observed in the untreated control cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C2A-GST%20and%20rodentia)]

Wang et al. (15) performed ex vivo biodistribution studies in normal mice (n = 3/group) at 15, 60, and 120 min after injection of 0.37 MBq (0.01 mCi) 4-[^18^F]FB-C2A-GST. The initial accumulation expressed as percent injected dose/gram (% ID/g) was high in the lung (~20% ID/g), liver (~15% ID/g), kidney (~12% ID/g), and spleen (~8% ID/g) at 15 min after injection and cleared rapidly afterwards with the exception of the kidney. The kidney accumulation was higher at the later time points (~20%–30% ID/g). The accumulation was low (<2% ID/g) in the heart, intestine, muscle, brain, and stomach. The blood radioactivity level was 0.95% ID/g at 120 min after injection. 4-[^18^F]FB-C2A-GST was 90% intact in the plasma at 120 min after injection. Dynamic PET scans with 4-[^18^F]FB-C2A-GST clearly visualized the liver, lungs, and heart during the first 10 min, at which point the radioactivity levels declined. On the other hand, the radioactivity level in the kidneys increased gradually with time. NO blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C2A-GST%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

Wang et al. (15) induced tumor apoptosis with a single dose of paclitaxel in rabbits (n = 6) bearing VX2 lung tumors in the right lung. PET imaging studies were performed with 4-[^18^F]FB-C2A-GST before paclitaxel treatment and at 72 h after paclitaxel treatment. PET imaging with [^18^F]FDG was also performed to confirm the presence of tumors before paclitaxel treatment. Little 4-[^18^F]FB-C2A-GST accumulation was found in the [^18^F]FDG-avid tumor lesions. However, intense 4-[^18^F]FB-C2A-GST accumulation was found in the tumor lesion. Standard uptake values were 0.47 ± 0.29 (n = 6) and 0.009 ± 0.001 (n = 2) for the paclitaxel-treated group and the untreated group (P < 0.001), respectively. Histological staining of tumor sections showed a significant increase (P < 0.001) in the number of apoptotic cells in the paclitaxel-treated group (80.0 ± 8.7%) compared with the number of apoptotic cells in the untreated group (5.0 ± 0.8%).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C2A-GST%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=C2A-GST%20and%20human)]

No publication is currently available.

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
3 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
4 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
5 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
6 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
7 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
8 Fernandez-Chacon R., Konigstorfer A., Gerber S.H., Garcia J., Matos M.F., Stevens C.F., Brose N., Rizo J., Rosenmund C., Sudhof T.C. (2001). Synaptotagmin I functions as a calcium regulator of release probability. Nature.
9 Davletov B.A., Sudhof T.C. (1993). A single C2 domain from synaptotagmin I is sufficient for high affinity Ca2+/phospholipid binding. J Biol Chem.
10 Audi S., Poellmann M., Zhu X., Li Z., Zhao M. (2007). Quantitative analysis of [99mTc]C2A-GST distribution in the area at risk after myocardial ischemia and reperfusion using a compartmental model. Nucl Med Biol.
11 Fang W., Wang F., Ji S., Zhu X., Meier H.T., Hellman R.S., Brindle K.M., Davletov B., Zhao M. (2007). SPECT imaging of myocardial infarction using 99mTc-labeled C2A domain of synaptotagmin I in a porcine ischemia-reperfusion model. Nucl Med Biol.
12 Liu Z., Zhao M., Zhu X., Furenlid L.R., Chen Y.C., Barrett H.H. (2007). In vivo dynamic imaging of myocardial cell death using 99mTc-labeled C2A domain of synaptotagmin I in a rat model of ischemia and reperfusion. Nucl Med Biol.
13 Wang F., Fang W., Zhao M., Wang Z., Ji S., Li Y., Zheng Y. (2008). Imaging paclitaxel (chemotherapy)-induced tumor apoptosis with 99mTc C2A, a domain of synaptotagmin I: a preliminary study. Nucl Med Biol.
14 Zhao M., Zhu X., Ji S., Zhou J., Ozker K.S., Fang W., Molthen R.C., Hellman R.S. (2006). 99mTc-labeled C2A domain of synaptotagmin I as a target-specific molecular probe for noninvasive imaging of acute myocardial infarction. J Nucl Med.
15 Wang F., Fang W., Zhang M.R., Zhao M., Liu B., Wang Z., Hua Z., Yang M., Kumata K., Hatori A., Yamasaki T., Yanamoto K., Suzuki K. (2011). Evaluation of chemotherapy response in VX2 rabbit lung cancer with 18F-labeled C2A domain of synaptotagmin I. J Nucl Med.